# Gadolinium 1-((11-S)-3,10-diaza-13-carboxamido-11-carboxy-2,9-dioxotridecyl)-N,N’,N”-tris(carboxymethyl)-1,4,7,10-tetraazacyclododecane

Chemical name: | Gadolinium 1-((11-S)-3,10-diaza-13-carboxamido-11-carboxy-2,9-dioxotridecyl)-N,N’,N”-tris(carboxymethyl)-1,4,7,10-tetraazacyclododecane
Abbreviated name: | Gd-DOTAMA-C6-Gln
Synonym:
Agent category: | Small molecule
Target: | Glutamine transporter
Target category: | Transporter
Method of detection: | Magnetic Resonance Imaging (MRI)
Source of signal/contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Gd-DOTAMA-C6-Gln))]

Malignant cells that precede rapid cellular proliferation require an increasing supply of precursor amino acids to support protein and nucleotide biosynthesis (1). These substrates are translocated from the blood stream into cytoplasma (internalization) via highly efficient transporters that belong to a group of carrier proteins residing in the plasma membrane. After entering the cytoplasma, glutamine (Gln) is further transported into the mitochondria and hydrolyzed by phosphate-dependent glutaminase (2). As a main source of nitrogen, Gln circulates in the blood stream at 0.6–0.9 mmol/L and accumulates in some tissues in concentrations as high as 20 mmol/L (2). Tumors compete with surrounding tissues for nitrogen compounds, producing a negative nitrogen balance in host tissues and substantial nitrogen increase in tumors (3). Therefore, the evaluation of protein metabolism can be carried out via imaging of the Gln uptake in tumors (4, 5). Because the internalization of Gln is mediated by Na^+^-dependent amino acid transporters, attaching a small gadolinium (Gd) chelate to Gln should not interfere with this receptor-mediated endocytosis process (RME) (5, 6). Although receptors normally are found in concentrations of 10^-9^ to 10^-13^ mol/g of tissue (1 μM to 10^-4^ μM), the RME mechanism recycles the receptor rapidly and results in a substantial ligand accumulation inside a cell in a short time (7). As an example, the ligands can be enriched to 10^-8^ to 10^-9^ mol/g in 1 h (7). For Gd chelates, this concentration meets the minimum requirement for magnetic resonance imaging (MRI) detection (8). The Gln transportation rate for tumors like hepatoma is 10–20 times faster than that for the healthy hepatocytes (1). Thus, the difference in Gln uptake can be used to distinguish between tumors and tissues via contrast agent–enhanced MRI (5).

Gadolinium 1-((11-S)-3,10-diaza-13-carboxamido-11-carboxy-2,9-dioxotridecyl)-N,N’,N”-tris(carboxymethyl)-1,4,7,10-tetraazacyclododecane (Gd-DOTAMA-C6-Gln) is a functionalized Gln in which the amino group is linked to a Gd-1,4,7,10-tetraazacyclododecane-N,N’,N”,N”’- tetraacetic monoamide (Gd-DOTA) through a linear aliphatic chain of six carbons (-C_6_H_12_-) (5). Gd-DOTA moiety has a high thermodynamic stability that protects against the in vivo release of Gd ions (9). The aliphatic chain serves as a spacer between the DOTA coordination cage and the Gln moiety to reduce the hindrance of the whole complex and improve the interaction between the Gln moiety and the receptor on the cell membrane (5). The conjugation of Gd chelate to the amino group sacrifices one of the four Gln recognition points on its transporting proteins and prevents the transporting protein from proceeding with the successive steps that bring the Gln into the mitochondria (5). Thus, the transporter may move the Gd-DOTAMA-C6-Gln to the clathrin-rich region, where the chelates are trapped in the endosomal vesicles. The entrapment can cause a quenching effect in the relaxation enhancement because the endosomal membrane forms barriers for water molecules to interact with the paramagnetic centers (5). The small size of DOTAMA-C6-Gln allows for easy extravasation and diffusion into the tissue to reach the surface of tumor cells.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Gd-DOTAMA-C6-Gln)+AND+synthesis%0D%0A)]

Crich et al. reported a detailed synthesis of Gd-DOTAMA-C6-Gln (5). DOTAMA-C6-Gln was obtained by a coupling reaction between the N-hydroxysuccinimide (NHS) activated ester of 1-(3-aza-8-carboxy-2-oxooctyl)-N,N’,N”-tris((1,1-dimethylethoxy)carbonylmethyl)-1,4,7,10-tetraazacyclododecane (DOTAMA(tBuO)_3_-(CH_2_)_6_-OH) and the unprotected L-glutamine in a homogeneous mixture of acetonitrile and a phosphate buffer (pH 8). After deprotection of the tert-butyl esters in the presence of trifluoroacetic acid and CH_2_Cl_2_ (1:1) at 50% yield, the purified ligand formed a complex with GdCl_3_ (pH 6.5).

The precursor 1-(3-aza-8-carboxy-2-oxooctyl)-4,7,10-tris(1,1-dimethylethoxy)-1,4,7,10-tetraazacyclododecane NHS (DOTAMA(tBuO)_3_-(CH_2_)_6_-NHS) was prepared in multiple steps. First, 6-aminohexanoic acid benzyl ester was reacted with bromoacetyl bromide in the presence of K_2_CO_3_ in acetonitrile to yield 7-aza-9-bromo-8-oxononanoic acid benzyl ester at 90% yield. This product was converted to 1-(3-aza-8-carboxy-2-oxooctyl)-N,N’,N”-tris((1,1-dimethylethoxy)carbonylmethyl)-1,4,7,10-tetraazacyclododecane benzyl ester at 96.5% yield by reacting it with 1,4,7,10-tetraazacyclododecane-N,N’,N”-tris-tert-butylester (DO3A-tris-tert-butylester) in the presence of K_2_CO_3_ in acetonitrile. Then, the ester was hydrogenated in methanol under catalyzation of 10% Pd/C to produce DOTAMA(tBuO)_3_-(CH_2_)_6_-OH in 50% yield, which was further converted to DOTAMA-(CH_2_)_6_-NHS by reacting with NHS in CH_2_Cl_2_.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(GD-DOTAMA-C6-Gln)+AND+%22in+vitro%22)]

The relaxation properties of water were examined with ^1^H nuclear magnetic resonance (NMR) dispersion spectroscopy (NMRD) at different magnetic field strengths and with ^17^O NMR spectroscopy at different temperatures (5). The structural water residual time (τ_m_) was found to be 1.5 μs at 25°C, and the electronic relaxation time (τ_v_) and the rotation correlation time (τ_R_) were 25 and 83 ps, respectively. The T_1_ relaxivity was found to be 5.5 mM^-1^s^-1^ at 0.47 T and 25°C in aqueous solution. For hepatoma cellular pellets with internalized Gd-DOTAMA-C6-Gln, the T_1_ relaxivity was measured as a function of Gd per cell, which exhibited a substantial deviation from the theoretical calculation. This indicated that the internalization of the chelates occurred through the entrapment into endosomal vesicles.

The uptake of Gd-DOTAMA-C6-Gln in cells was tested in healthy rat hepatocytes, rat hepatoma cells (HTC), rat glioma C6 cells, murine breast adenocarcinoma cells (TSA), and murine neuroblastoma cells (Neuro-2a) (5). Two to three million cells were incubated for 6 h at 37°C in Earl’s balanced salt solution (EBSS) containing Gd-DOTAMA-C6-Gln at 1.6 mM (three times higher than the glutamine physiological concentration). After incubation, the cells were washed three times and then destroyed. The Gd was released from the cells as free aquo-ions and quantified by inductively coupled plasma mass spectrometry (ICP-MS) to determine internalized Gd content (10). For all tumor cells, the internalized Gd was found to be >1 × 10^-8^ mol Gd /mg cell protein. The uptake of Gd-DOTAMA-C6-Gln by HTC cells appeared to decrease markedly as the concentration of the free Gln added to the culture medium increased. This result also demonstrated that Gln residue present on the surface of Gd-DOTAMA-C6-Gln complex was the vehicle for the internalization through the amino transporting system. The Gd-DOTAMA-C6-Gln uptake for HTC cells was further compared with that for hepatocytes by in vitro MRI on a 7-T imager. After 4 h of incubation in 1.6 mM of Gd-DOTAMA-C6-Gln, 23 nmol of Gd/mg cell protein was found in HTC cells, which was four times higher than the 5.5 nmol of Gd/mg cell protein in the hepatocytes. This difference was also reflected in the T_1_-weighted images on which a 45% increase in signal intensity was found for the HTC cells compared to the healthy hepatocytes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Gd-DOTAMA-C6-Gln) +AND++rodentia)]

MRI experiments were conducted to distinguish between tumors and normal tissues in two rodent tumor models (5). A dose of Gd-DOTAMA-C6-Gln (0.2 mmol/kg) was injected intravenously into A/J mice grafted with Neuro-2a and her-2/neu transgenic mice with mammary carcinoma. From 24 to 72 hr after injection, T_1_-weighted images were acquired on a 7-T imager when the renal elimination of the non-internalized Gd complex was complete. The tumor signal intensity (SI) was significantly high, indicating that the amount of internalized Gd complex was sufficient to yield a substantial enhancement effect. The SI enhancement was homogeneously distributed in the tumor mass and was more pronounced in tumors with a diameter <3 mm. In comparison, the kidney cortical region showed ~15% SI enhancement. For the transgenic mouse model, the Gd uptake in the her-2/neu tumors was determined by ICP-MS. Tumors were extracted by euthanizing the mice 24 h after injection. The amount of Gd-DOTAMA-C6-Gln in tumors was found to be 2.1 ± 0.4 nmol Gd/g protein in tumors <3 mm in diameter and 1.2 ± 0.4 nmol Gd/g protein in tumors >3 mm in diameter. Compared to the muscles, the uptake of Gd-DOTAMA-C6-Gln was seven- to eight-fold higher for tumors <3 mm in diameter and four-fold higher for tumors >3 mm in diameter.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Gd-DOTAMA-C6-Gln) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Gd-DOTAMA-C6-Gln) +AND+human)]

No publication is currently available.

## References

1 Wasa M., Bode B.P., Abcouwer S.F., Collins C.L., Tanabe K.K., Souba W.W. (1996). Glutamine as a regulator of DNA and protein biosynthesis in human solid tumor cell lines. Ann Surg.
2 Souba W.W. (1993). Glutamine and cancer. Ann Surg.
3 Medina M.A., Sanchez-Jimenez F., Marquez J., Rodriguez Quesada A., Nunez de Castro I. (1992). Relevance of glutamine metabolism to tumor cell growth. Mol Cell Biochem.
4 Lattuada L., Demattio S., Vincenzi V., Cabella C., Visigalli M., Aime S., Crich S.G., Gianolio E. (2006). Magnetic resonance imaging of tumor cells by targeting the amino acid transport system. Bioorg Med Chem Lett.
5 Geninatti Crich S., Cabella C., Barge A., Belfiore S., Ghirelli C., Lattuada L., Lanzardo S., Mortillaro A., Tei L., Visigalli M., Forni G., Aime S. (2006). In vitro and in vivo magnetic resonance detection of tumor cells by targeting glutamine transporters with Gd-based probes. J Med Chem.
6 Conti F., Melone M. (2006). The glutamine commute: lost in the tube?. Neurochem Int.
7 Nunn A.D., Linder K.E., Tweedle M.F. (1997). Can receptors be imaged with MRI agents?. Q J Nucl Med.
8 Ahrens E.T., Rothbacher U., Jacobs R.E., Fraser S.E. (1998). A model for MRI contrast enhancement using T1 agents. Proc Natl Acad Sci U S A.
9 Bousquet J.C., Saini S., Stark D.D., Hahn P.F., Nigam M., Wittenberg J., Ferrucci J.T. (1988). Gd-DOTA: characterization of a new paramagnetic complex. Radiology.
10 Crich S.G., Biancone L., Cantaluppi V., Duo D., Esposito G., Russo S., Camussi G., Aime S. (2004). Improved route for the visualization of stem cells labeled with a Gd-/Eu-chelate as dual (MRI and fluorescence) agent. Magn Reson Med.